# 16α-[^18^F]Fluoro-17β-estradiol

Chemical name: | 16α-[^18^F]Fluoro-17β-estradiol
Abbreviated name: | [^18^F]FES
Synonym: | 16-Fluoroestradiol, fluoroestradiol
Agent category: | Compound
Target: | Estrogen receptor
Target category: | Receptor
Method of detection: | PET
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2216-fluoroestradiol%22%5BSubstance%20Name%5D)]

Estrogens and progestins are endogenous hormones that produce many physiological effects. Estrogens act primarily by regulating gene expression. Estrogen receptors are found in the cell nucleus of the female reproductive tract, breast, pituitary, hypothalamus, bone, liver, and other tissues, and also in various tissues in men. Estrogens are lipophilic that they enter the cell passively by diffusion through the cellular membrane. They bind to estrogen receptors that are present in the nucleus.

Breast cancer is the most common malignancy in women. About 33% of women who have this disease will die of disseminated breast cancer. The growth of breast epithelial cells is dependent on estrogen stimulation to induce progestin receptor expression. Two-thirds of breast carcinomas express ERs. It has also been established that the ER status of the tumor is an important prognostic indicator in breast cancer (1). Women with ER-positive breast tumors have a better prognosis than women with ER-negative tumors in terms of responsiveness to anti-estrogen treatment. ER content in breast cancer was assessed by receptor binding assays, which suffer from inter-assay variability and are also limited by intrinsic receptor heterogeneity of the tumor. 16α-[^18^F]Fluoro-17β-estradiol ([^18^F]FES) was proven to be a valuable tracer for the studies of the ER status of primary and metastatic breast cancer (2).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2216-fluoroestradiol%22%5BSubstance%20Name%5D%20AND%20synthesis)]

[^18^F]FES was first synthesized by nucleophilic displacement of the aliphatic triflate of 3,16β-bis(trifluoromethenesulfonyloxy)estrone using tetrabutylammonium [^18^F]fluoride, followed by hydrolysis and ketone reduction. High-performance liquid chromatography (HPLC) purification provided a 30% radiochemical yield of [^18^F]FES in about 90 min (3). On the basis of this method, an automated robotic synthesis was developed to give an overall yield of 6% in 80 min (4). A one-pot synthesis of [^18^F]FES was synthesized by nucleophilic fluorination of 3-methoxymethyl-16β,17β-epiestriol-O-cyclic sulfone. [^18^F]FES was isolated to provide radiochemical yields of 30-45% with a specific activity of about 37 GBq/µmol (1 Ci/µmol) in 60-120 min (5). Automated modules were developed for the synthesis of [^18^F]FES to give ~50% radiochemical yields in 50-80 min (6, 7). Recently, automated synthesis procedure has been developed for clinical large-scale production of [^18^F]FES in good yields (15-35%) with high radiochemical purity (>99%) (8).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2216-fluoroestradiol%22%5BSubstance%20Name%5D%20AND%20in%20vitro)]

ER binding affinity was assessed by competitive binding with [^3^H]estradiol in MCF-7 cells. The binding affinity of FES was about 57% of estradiol (9). FES showed little binding to sex hormone-binding globulin as compared to estradiol.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2216-fluoroestradiol%22%5BSubstance%20Name%5D%20AND%20rodentia)]

It was demonstrated that [^18^F]FES uptake by target tissues (uterus and ovary) in immature female rats is highly specific (10). The uptake in liver and kidneys was lower than the uterus and nonspecific. There was also a significant depression of [^18^F]FES uptake by the target tissues after pretreatment with the anti-estrogen, tamoxifen. [^18^F]FES uptake by rat 7,12-dimethylbenz[a]anthracene (DMBA)-induced breast tumors correlated well with the ER concentration (11). In another study, it was found that metabolism of [^18^F]FES was rapid in rats bearing DMBA-induced breast tumors within 1-2 h after injection. Most of the radioactivity in the blood and non-target tissues was [^18^F]FES metabolites, which did not bind to the target tissues and breast tumors (12).

Different animal models of estrogen-positive tumors using [^18^F]FES were evaluated for their suitability to follow tumor response after various treatment protocols, using small-animal positron emission tomography (PET) (13). ER-positive human breast cancer cell lines MCF-7 and T-47D and murine mammary carcinomas MC4-L2, MC4-L3, and MC7-L1 were compared for their in vivo growth rate and retention of ER-positive status. Tumor metabolic activity was estimated from [^18^F]fluorodeoxyglucose ([^18^F]FDG) uptake, whereas ER content was determined from [^18^F]FES uptake. The human cell lines grew at a slower rate in nude mice and failed to accumulate [^18^F]FES; in contrast, the MC7-L1 and MC4-L2 carcinomas grew well in mice and showed good uptake of both [^18^F]FDG and [^18^F]FES. Chemotherapy and hormone therapy delayed the growth of MC7-L1 and MC4-L2 tumors, confirming their suitability as an ER-positive model for therapeutic interventions. The murine MC7-L1 and MC4-L2 tumors are suitable models for the monitoring of ER-positive breast cancer therapy using small-animal PET imaging.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2216-fluoroestradiol%22%5BSubstance%20Name%5D%20AND%20%28dog%20or%20pig%20or%20rabbit%20or%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2216-fluoroestradiol%22%5BSubstance%20Name%5D%20AND%20primates%20not%20humans)]

No relevant publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2216-fluoroestradiol%22%5BSubstance%20Name%5D%20AND%20human)]

Thirteen patients with primary breast lesions were studied with [^18^F]FES PET (14). PET images demonstrated uptake of the tracer at sites of primary tumors and in several axillary lymph node metastases, as well as in one distant metastatic lesion. There was an excellent correlation between uptake within the primary tumor measured on the PET images and the tumor ER concentration measured by in vitro receptor binding assays after excision (r = 0.96). In a study with 15 breast cancer patients (15), [^18^F]FES was cleared from the blood and metabolized in 20 min with only 20% of intact [^18^F]FES, most of which was bound to plasma proteins. Liver uptake of [^18^F]FES was rapid, and [^18^F]FES metabolites appeared in the blood as early as 5 min. The major, labeled metabolites in the blood and urine were sulfate and glucuronidate conjugates of [^18^F]FES, as measured by HPLC.

Human dosimetry of [^18^F]FES was determined from blood samples and PET images in 49 patients after intravenous injection of [^18^F]FES (16).The effective dose equivalent was 0.022 mSv/MBq (80 mrem/mCi). The organ that received the highest dose was the liver (0.13 mGy/MBq (470 mrad/mCi)), followed by the gallbladder (0.10 mGy/MBq (380 mrad/mCi)) and the urinary bladder (0.05 mGy/MBq (190 mrad/mCi)).

Uptake of [^18^F]FES in a series of patients with primary breast lesions and recurrent/metastatic breast tumors was compared with in vitro ER content and tumor uptake of [^18^F]FDG (17). There was no correlation between tumor ER status and [^18^F]FDG uptake or between tumor [^18^F]FES and [^18^F]FDG uptake in these patients. However, the [^18^F]FES PET assessments were in agreement with the in vitro ER binding assays. Anti-estrogen therapy decreased [^18^F]FES uptake in patients with ER-positive lesions (18), and patients with high initial uptake of [^18^F]FES were more likely to respond favorably to hormonal therapy (19). Peterson et al. (20) studied seventeen patients with primary or metastatic breast cancer with dynamic [^18^F]FES PET. For each tumor, partial-volume-corrected standardized uptake values (SUVs) of [^18^F]FES uptake were compared with ER expression measured by 3 different ER scoring methods: qualitative scoring, the Allred score , and a computerized immunohistochemistry (IHC) index. There was excellent agreement (r = 0.99) between observers using IHC as well as the different methods of measuring ER content (P < 0.001) with the best correlation being between the IHC index and [^18^F]FES SUVs. Tumor imaging with [^18^F]FES PET is useful in the determination of ER status and prognosis of therapy in breast cancer patients [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2216-fluoroestradiol%22%5BSubstance%20Name%5D%20AND%20%22humans%22%5BMeSH%20Terms%5D%20AND%20%22breast%20neoplasms%22%5BMeSH%20Terms%5D)].

## NIH Support

CA25836, CA42045, CA48286, CA72064, CA72964, DK15556, HL13851, RR17229

## References

1 Vollenweider-Zerargui L., Barrelet L., Wong Y., Lemarchand-Beraud T., Gomez F. (1986). The predictive value of estrogen and progesterone receptors' concentrations on the clinical behavior of breast cancer in women. Clinical correlation on 547 patients. Cancer.
2 Flanagan F.L., Dehdashti F., Siegel B.A. (1998). PET in breast cancer. Semin Nucl Med.
3 Kiesewetter D.O., Kilbourn M.R., Landvatter S.W., Heiman D.F., Katzenellenbogen J.A., Welch M.J. (1984). Preparation of four fluorine- 18-labeled estrogens and their selective uptakes in target tissues of immature rats. J Nucl Med.
4 Brodack J.W., Kilbourn M.R., Welch M.J., Katzenellenbogen J.A. (1986). Application of robotics to radiopharmaceutical preparation: controlled synthesis of fluorine-18 16 alpha-fluoroestradiol-17 beta. J Nucl Med.
5 Lim J.L., Zheng L., Berridge M.S., Tewson T.J. (1996). The use of 3-methoxymethyl-16 beta, 17 beta-epiestriol-O-cyclic sulfone as the precursor in the synthesis of F-18 16 alpha-fluoroestradiol. Nucl Med Biol.
6 Oh S.J., Chi D.Y., Mosdzianowski C., Kil H.S., Ryu J.S., Moon D.H. (2007). The automatic production of 16alpha-[18F]fluoroestradiol using a conventional [18F]FDG module with a disposable cassette system. Appl Radiat Isot.
7 Romer J., Fuchtner F., Steinbach J., Kasch H. (2001). Automated synthesis of 16alpha-[18F]fluoroestradiol-3,17beta-disulphamate. Appl Radiat Isot.
8 Kumar P., Mercer J., Doerkson C., Tonkin K., McEwan A.J. (2007). Clinical production, stability studies and PET imaging with 16-alpha-[18F]fluoroestradiol ([18F]FES) in ER positive breast cancer patients. J Pharm Pharm Sci.
9 Seimbille Y., Rousseau J., Benard F., Morin C., Ali H., Avvakumov G., Hammond G.L., van Lier J.E. (2002). 18F-labeled difluoroestradiols: preparation and preclinical evaluation as estrogen receptor-binding radiopharmaceuticals. Steroids.
10 Katzenellenbogen J.A., Mathias C.J., VanBrocklin H.F., Brodack J.W., Welch M.J. (1993). Titration of the in vivo uptake of 16 alpha-[18F]fluoroestradiol by target tissues in the rat: competition by tamoxifen, and implications for quantitating estrogen receptors in vivo and the use of animal models in receptor-binding radiopharmaceutical development. Nucl Med Biol.
11 Sasaki M., Fukumura T., Kuwabara Y., Yoshida T., Nakagawa M., Ichiya Y., Masuda K. (2000). Biodistribution and breast tumor uptake of 16alpha-[18F]-fluoro-17beta-estradiol in rat. Ann Nucl Med.
12 Mathias C.J., Welch M.J., Katzenellenbogen J.A., Brodack J.W., Kilbourn M.R., Carlson K.E., Kiesewetter D.O. (1987). Characterization of the uptake of 16 alpha-([18F]fluoro)-17 beta-estradiol in DMBA-induced mammary tumors. Int J Rad Appl Instrum B.
13 Aliaga A., Rousseau J.A., Ouellette R., Cadorette J., van Lier J.E., Lecomte R., Benard F. (2004). Breast cancer models to study the expression of estrogen receptors with small animal PET imaging. Nucl Med Biol.
14 Mintun M.A., Welch M.J., Siegel B.A., Mathias C.J., Brodack J.W., McGuire A.H., Katzenellenbogen J.A. (1988). Breast cancer: PET imaging of estrogen receptors. Radiology.
15 Mankoff D.A., Tewson T.J., Eary J.F. (1997). Analysis of blood clearance and labeled metabolites for the estrogen receptor tracer [F-18]-16 alpha-fluoroestradiol (FES). Nucl Med Biol.
16 Mankoff D.A., Peterson L.M., Tewson T.J., Link J.M., Gralow J.R., Graham M.M., Krohn K.A. (2001). [18F]fluoroestradiol radiation dosimetry in human PET studies. J Nucl Med.
17 Dehdashti F., Mortimer J.E., Siegel B.A., Griffeth L.K., Bonasera T.J., Fusselman M.J., Detert D.D., Cutler P.D., Katzenellenbogen J.A., Welch M.J. (1995). Positron tomographic assessment of estrogen receptors in breast cancer: comparison with FDG-PET and in vitro receptor assays. J Nucl Med.
18 McGuire A.H., Dehdashti F., Siegel B.A., Lyss A.P., Brodack J.W., Mathias C.J., Mintun M.A., Katzenellenbogen J.A., Welch M.J. (1991). Positron tomographic assessment of 16 alpha-[18F] fluoro-17 beta-estradiol uptake in metastatic breast carcinoma. J Nucl Med.
19 Dehdashti F., Flanagan F.L., Mortimer J.E., Katzenellenbogen J.A., Welch M.J., Siegel B.A. (1999). Positron emission tomographic assessment of "metabolic flare" to predict response of metastatic breast cancer to antiestrogen therapy. Eur J Nucl Med.
20 Peterson L.M., Mankoff D.A., Lawton T., Yagle K., Schubert E.K., Stekhova S., Gown A., Link J.M., Tewson T., Krohn K.A. (2008). Quantitative imaging of estrogen receptor expression in breast cancer with PET and 18F-fluoroestradiol. J Nucl Med.